# 2’-[^18^F]Fluorofolic acid

Chemical name: | 2’-[^18^F]Fluorofolic acid
Abbreviated name: | 2’-[^18^F]FFA
Synonym:
Agent category: | Compound
Target: | Putative folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate)]

Folic acid is a water-soluble vitamin B_9_ (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Epithelial cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a receptor on the cell membrane with higher affinity (dissociation constant (K_d_) = 0.5 nM), which allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate-binding protein (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the corresponding normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have also been found to have the folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate, and ^68/67/66^Ga-DF-folate (http://www.ncbi.nlm.nih.gov/books/NBK23092/)) have been studied in tumor imaging (4-7). Bettio et al. (8) reported a synthesis of ^18^F-labeled folate by reaction of [^18^F]4-fluorobenzylamine (FBA) with the α- and γ-carboxyl groups of folic acid. [^18^F]α/γ-FBA-folate (http://www.ncbi.nlm.nih.gov/books/NBK23020/) has been evaluated as a positron emission tomography (PET) agent for detection of folate receptors in tumors in mice. However, the low radiochemical yield from multistep radiosynthesis limited its routine use. Ross et al. (9) introduced the ^18^F label at the 2’ position of the 4-amino-benzoyl moiety in folic acid to form 2’-[^18^F]fluorofolic acid (2’-[^18^F]FFA). 2’-[^18^F]FFA was found to be a specific, high-affinity PET agent for imaging folate receptor-positive tumors in mice.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptors (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20synthesis)]

Ross et al. (9) prepared 2’-[^18^F]FFA with a two-step synthesis using a standard nucleophilic radiofluorination ([^18^F]KF/Kryptofix 2.2.2) reaction of N^2^-(N,N-dimethylaminomethylene)-2'-nitrofolic acid di-tert-butylester (8 µmol) (140ºC, 20 min) and subsequent acid hydrolysis (60ºC, 12 min). Maximal overall decay-corrected yield was 4% with >95% radiochemical purity. The total synthesis time was 80 min, and the specific activity was 23.7 ± 12.2 GBq/µmol (0.64 ± 0.33 Ci/µmol). The relative lipophilicity (retention factor, k’) of 2’-FFA as determined with high-performance liquid chromatography was 0.53 as compared to 0.30 for folic acid.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB cell line has putative folate receptors as determined with [^3^H]folate binding studies in cultures (8). The mean 50% inhibition concentrations for 2’-FFA and folic acid were 3.4 ± 0.3 and 1.1 ± 0.4 nM (9), respectively. Therefore, 2’-FFA has a binding affinity comparable to that of native folic acid.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20rodentia)]

Ross et al. (9) performed biodistribution studies of 1 MBq (0.027 mCi) 2’-[^18^F]FFA in nude mice (n = 4) bearing KB tumor xenografts. The organ with the highest accumulation at 75 min after injection was the kidney (46.06% injected dose/gram (ID/g)), followed by the gallbladder (17.69% ID/g), tumor (9.37% ID/g), liver (7.79% ID/g), and intestine (2.80% ID/g). Very high radioactivity was found in the urine. The radioactivity levels in the blood and bone were 0.40% ID/g and 1.59% ID/g, respectively. Accumulation in the brain, lung, heart, spleen, and stomach was <2% ID/g. There was ~33% intact 2’-[^18^F]FFA in the plasma and tumor at 15 min after injection with one major hydrophilic metabolite. Pretreatment with folic acid (200 μg/mouse) 10 min before 2’-[^18^F]FFA injection reduced 2’-[^18^F]FFA accumulation by 90% in the brain, 83% in the tumor, and 81% in the kidney. Less reduction was observed in the lung, heart, spleen, and stomach.

The whole-body distribution of 2’-[^18^F]FFA was also assessed with PET imaging 75–105 min after injection. High accumulation was visualized in the kidneys, gallbladder, urinary bladder, tumor, and intestines. Moderate accumulation was observed in the liver. The accumulation of 2’-[^18^F]FFA in the tumor and kidneys was reduced to near background level after folic acid pretreatment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Ross T.L., Honer M., Muller C., Groehn V., Schibli R., Ametamey S.M. (2010). A new 18F-labeled folic acid derivative with improved properties for the PET imaging of folate receptor-positive tumors. J Nucl Med.